# ^99m^Tc-Acetyl-Asn-Gln-Glu-Gln-Val-Ser-Pro-3-iodo-Tyr-Thr-Leu-Leu-Lys-Gly-NC100194

Chemical name: | ^99m^Tc-Acetyl-Asn-Gln-Glu-Gln-Val-Ser-Pro-3-iodo-Tyr-Thr-Leu-Leu-Lys-Gly-NC100194
Abbreviated name: | ^99m^Tc-NC100668
Synonym:
Agent Category: | Polypeptide
Target: | Activated coagulation factor XIIIa (FXIIIa)
Target Category: | Covalently linked to fibrin
Method of detection: | SPECT, planar
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=119720), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=119395708) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=281757) for more information about coagulation factor XIIIa.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NC100668)]

Thrombosis plays a major role in many cardiovascular diseases such as myocardial infarction, pulmonary embolism, deep venous thrombosis, or cerebral venous thrombosis (1). Thrombosis occurs by an activation process of thrombin, which then converts fibrinogen into fibrin. Thrombin initiates the cross-linking of the polymerized fibrin via the activation of a transglutamase enzyme called coagulation factor XIII (FXIIIa indicates activated factor XIII) (2). FXIIIa increases acute thrombus stability by rapidly cross-linking a lysine residue in fibrin α- and γ-chains to a glutamine residue in α-2 antiplasmin. FXIIIa has an in vivo catalytic half-life (t_½_) of ~20 min (3).

NC100668 (Acetyl-Asn-Gln-Glu-Gln-Val-Ser-Pro-3-iodo-Tyr-Thr-Leu-Leu-Lys-Gly-NC100194) is a probe that is recognized by the enzyme FXIIIa and covalently binds to fibrin by means of the transglutamase activity of FXIIIa (4, 5). NC100194 (N,N-bis(N-(1,1-dimethyl-2-(hydroxylimino-)propyl)aminoethyl)aminoethylamine) is a ^99m^Tc-chelator. Single-photon emission computed tomography (SPECT) imaging with an FXIIIa probe may be a useful tool in the diagnosis of thrombosis and may provide valuable information currently unavailable through anatomically-based imaging modalities.

Preliminary research has shown that ^99m^Tc-NC100668 is capable of measuring the activity of FXIIIa and visualizing thrombus in vivo (6, 7). ^99m^Tc-NC100668 may be used as a molecular diagnostic tool for therapy with fibrinolytic or anti-FXIIIa inhibitors, and other drugs for diseases such as cerebral venous thrombosis, ischemic stroke, or myocardial infarction. Additional and more extensive research studies are needed to fully assess the potential application of the ^99m^Tc-NC100668 imaging modality.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NC100668%20and%20synthesis)]

^99m^Tc-NC100668 was prepared from commercially available lyophilized kits. A solution of 2.5 GBq (68 mCi) sodium pertechnetate (^99m^Tc) was added to a vial containing 100 μg NC100668 and heated at 60–65ºC for 10–12 min. Radiochemical purity was determined by high-performance liquid chromatography to be >89% with a major impurity of 6% as an isomer of ^99m^Tc-NC100668. Specific activity and radiochemical yield were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NC100668%20and%20in%20vitro)]

Edwards et al. (6) reported that ^99m^Tc-NC100668 was >90% intact after 90 min of incubation in saline and rat plasma and >70% in rat blood. The uptake of ^99m^Tc-NC100668 into rat, rabbit, dog, and human plasma clots (n = 12) was 36.9 ± 0.5%, 53.4 ± 16.7%, 57.1 ± 6.3%, and 56.7 ± 2.5%, respectively (7). The uptake of ^99m^Tc-AH110563 (an inactive NC100668 analog) into human plasma clot was only 1%. On the other hand, the uptake of the FXIIIa substrate ^14^C-labeled dansyl cadaverine was 11.4 ± 3.6%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NC100668%20and%20rodentia)]

Edwards et al. (7) performed biodistribution studies of ^99m^Tc-NC100668 in healthy rats (55 MBq/rat (1.49 mCi/rat)). The highest radioactivity concentrations, expressed as % injected dose (ID), were observed in the muscle (25% ID), blood (20% ID), kidneys (18% ID), skin (15% ID), fat (5% ID), urinary bladder (4% ID), liver (4% ID), and lungs (2% ID) at 2 min after injection. With the exception of the kidneys, all other organs and tissues showed a continuing decrease in radioactivity with time. The radioactivity in the urinary bladder was 44% ID at 20 min and 66% ID at 60 min.

Edwards et al. (7) performed biodistribution studies of ^99m^Tc-NC100668 in rats bearing an inferior vena cava blood clot that was 60 min old. The kidneys had the highest accumulation at 60 min after tracer injection (29% ID), followed by the urinary bladder (19% ID), muscle (11% ID), and blood (5% ID). The blood clot showed 0.11 ± 0.09% ID. The radioactive concentration ratio of ^99m^Tc in the blood clot to that in blood (9:1), muscle (31:1), and lung (15:1) demonstrated that ^99m^Tc-NC100668 was preferentially concentrated in the blood clot compared with these tissues. On the other hand, there was no specific accumulation of ^99m^Tc-AH110563 in the blood clot (0.01 ± 0.04% ID). With the exception of the kidneys, ^99m^Tc-NC100668 biodistribution and blood clot uptake are unaffected by the presence of 20-, 100-, and 1,000-fold excess of NC100668 (8), heparin, or thrombin inhibitor (9). The kidney retention of radioactivity is probably because of FXIIIa transglutaminase activity, which can be displaced by unlabeled NC100668. In contrast, the blood clot is able to recruit FXIIIa from activated platelets, and therefore accumulation of ^99m^Tc-NC100668 is not affected by 1,000-fold excess of NC100668.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NC100668%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NC100668%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NC100668%20and%20human)]

No publication is currently available.

## References

1 Corti R., Fuster V. (2003). New understanding, diagnosis, and prognosis of atherothrombosis and the role of imaging. Am J Cardiol.
2 Lee K.N., Lee C.S., Tae W.C., Jackson K.W., Christiansen V.J., McKee P.A. (2001). Crosslinking of alpha 2-antiplasmin to fibrin. Ann N Y Acad Sci.
3 Robinson B.R., Houng A.K., Reed G.L. (2000). Catalytic life of activated factor XIII in thrombi. Implications for fibrinolytic resistance and thrombus aging. Circulation.
4 Ichinose A. (2005). Extracellular transglutaminase: factor XIII. Prog Exp Tumor Res.
5 Jaffer F.A., Tung C.H., Wykrzykowska J.J., Ho N.H., Houng A.K., Reed G.L., Weissleder R. (2004). Molecular imaging of factor XIIIa activity in thrombosis using a novel, near-infrared fluorescent contrast agent that covalently links to thrombi. Circulation.
6 Edwards D., Battle M., Lear R., Farrar G., Barnett D.J., Godden V., Coombes C., Oliveira A., Ahlstrom H. (2006). The in vivo and in vitro metabolic profile of 99mTc-NC100668, a new tracer for imaging venous thromboembolism: identification and biodistribution of the principal radiolabeled metabolite. Drug Metab Dispos.
7 Edwards D., Lewis J., Battle M., Lear R., Farrar G., Barnett D.J., Godden V., Oliveira A., Coombes C., Ahlstrom H. (2006). (99m)Tc-NC100668, a new tracer for imaging venous thromboemboli: pre-clinical biodistribution and incorporation into plasma clots in vivo and in vitro. Eur J Nucl Med Mol Imaging.
8 Edwards D., Lewis J., Battle M., Lear R., Farrar G., Barnett D.J., Godden V., Edwards C., Oliveira A., Ahlstrom H. (2007). The biodistribution of NC100668 and the effect of excess NC100668 on the biodistribution and kidney retention of (99m)Tc-NC100668 in the rat. Nucl Med Biol.
9 Edwards D., Lewis J., Battle M., Lear R., Farrar G., Jon Barnett D., Godden V., Oliveira A., Coombes C., Ahlstrom H. (2007). 99mTc-NC100668, an agent for imaging venous thromboembolism: The effect of anticoagulant or thrombolytic therapy on the uptake and retention of radioactivity in blood clots in vivo. Nucl Med Commun.